# (+)-p-[^11^C]Methylvesamicolphenoxy)

Chemical name: | (+)-p-[^11^C]Methylvesamicol
Abbreviated name: | (+)-[^11^C]PMV
Synonym: | (+)-2-[4-(4-[^11^C]Methyl)phenylpiperidino]cyclohexanol
Agent Category: | Compound
Target: | Sigma (σ) receptor
Target Category: | Receptor binding
Method of detection: | Positron Emission Tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C%20PMV%20OR%20%28+%29-p-%5B%2811%29C%5D-methylvesamicol%20OR%20%28methyl%20vesamicol%29)]

(+)-p-[^11^C]Methylvesamicol ((+)-[^11^C]PMV) is a radioligand developed for positron emission tomography (PET) imaging of the sigma (σ) receptors. It is a sigma (σ) receptor ligand labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min (1).

σ receptors are functional, membrane-bound proteins distributed in the central nervous system (CNS) and peripheral organs (2). The CNS σ receptors are unique binding sites related to higher brain functions (3). They are distinct from opiate and phencyclidine (PCP) binding sites. There are at least two subtypes of σ receptors, σ_1_ and σ_2_ receptors. The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacologic and physiologic functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. PCP and derivatives, cocaine and derivatives, some neuroleptics, atyptical antipsychotic agents, and other chemically unrelated compounds can bind to the σ receptor sites. Studies have shown that these receptors may play a role in the pathogenesis of psychiatric disorders (4, 5).

The σ_1_ receptor subtypes appear to play a role in motor functions and potassium channels (2). The σ_2_ receptor subtypes are implicated in CNS disorders and malignant neoplastic diseases. Because of these effects, σ receptor ligands may be useful for detection and treatment in neurology and oncology. Matsuno et al. (6) developed a potent σ agonist, 1-(3,4-dimethoxyphenethyl)-4-(3-phenylpropyl)-piperazine dihydrochloride (SA4503), which is highly selective for σ_1_ receptors compared to σ_2_ receptors (6). SA4503 can be labeled with ^11^C or^18^F for PET studies of σ receptors (1, 7, 8). Another potential PET ligand is methylvesamicol, an analog of vesamicol. Vesamicol has been found to block the release of acetylcholine from cholinergic nerve terminals, and a number of radioiodine-, ^18^F-, and ^11^C-labeled vesamicol derivatives have been synthesized as PET or single-photon emission computed tomography (SPECT) radioligands to map vesicular cholinergic transporter (VAChT) sites (9, 10). Some of these vesamicol analogs have been shown to have moderate to high affinity for σ receptors (11, 12). Shiba et al. (13) showed that radiodinated (+)-p-iodovesamicol bound to σ_1_ receptors with high affinity and selectivity. In addition, Shiba et al. (12) reported that the (+)-enantiomer of methylvesamicol, (+)-PMV, had high affinity for the σ_1_ receptor and very low affinity for VAChT.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20PMV%20OR%20%28%20%29-p-%5B%2811%29C%5D-methylvesamicol%20OR%20%28methyl%20vesamicol%29%29%20AND%20synthesis)]

Shiba et al. (14) reported the synthesis of (+)-PMV from 4-(4-methylphenyl)piperidine. The 10-step reactions produced an overall yield of 1.3-4.1%. (+)-p-Tributylstannylvesamicol was used as the precursor of (+)-[^11^C]PMV prepared by a palladium-catalyzed reaction of the corresponding iodovesamicol. Radiosynthesis of (+)-[^11^C]PMV was performed by substituting the tributylstannyl group with [^11^C]methyl iodide in a palladium-promoted cross-coupling reaction (15). Briefly, [^11^C]methyl iodide was produced from [^11^C]CO_2_ and trapped in an N,N-dimethylformamide solution containing the precursor, tris(dibenzylideneacetone)dipalladium, tri(o-tolyl)phosphine, copper chloride, and potassium carbonate and then cooled by air. The reaction mixture was heated at 80ºC for 3 min. After the addition of ammonium acetate, the reaction mixture was filtered and purified by high-performance liquid chromatography (HPLC). The radiochemical yield was 7.7-19% based on [^11^C]methyl iodide, and the radiochemical purity was >97%. The specific activity of (+)-[^11^C]PMV was 41-162 TBq/mmol (1,107-4,374 Ci/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20PMV%20OR%20%28%20%29-p-%5B%2811%29C%5D-methylvesamicol%20OR%20%28methyl%20vesamicol%29%29%20AND%20in%20vitro)]

Shiba et al. (14) reported the in vitro binding affinities of (+)-PMV to the σ receptors and VAChT. In vitro competitive binding studies were conducted with (−)-[^3^H]vesamicol, (+)-[^3^H]pentazocine, or [^3^H]DTG in rat cerebral or liver membrane preparations. The K_i_ values (nM) were 3.0 ± 0.2, 40.7 ± 2.9, and 199 ± 32 for the σ_1_ receptor, the σ_2_ receptor, and VAChT, respectively. In comparison, SA4503 had K_i_ values of 4.4 ± 1.0, 242 ± 17, and 50.2 ± 7.2 for the σ_1_ receptor, the σ_2_ receptor, and VAChT, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20PMV%20OR%20%28%20+%29-p-%5B%2811%29C%5D-methylvesamicol%20OR%20%28methyl%20vesamicol%29%29%20AND%20rodentia)]

In a rat distribution study, an i.v. dose of 10 MBq/0.13 nmol (0.27 mCi/0.13 nmol) (+)-[^11^C]PMV was administered to each rat (15). The radioactivity levels (n = 4) in the brain were 0.97 ± 0.11, 0.96 ± 0.17, 1.00 ± 0.07, and 0.85 ± 0.08% injected dose (ID)/g at 5, 15, 30, and 60 min, respectively. The relative regional brain distribution was: cerebral cortex > cerebellum ≈ striatum > hippocampus. The striatum/cerebellum ratio decreased slightly from 1.01 ± 0.04 to 0.94 ± 0.05 at 60 min. In comparison, the ratio of [^11^C]SA4503 remained constant with 0.99 ± 0.05 at 5 min and 1.03 ± 0.02 at 60 min. Pretreatment with 50 μmol/kg of (±)-pentazocine reduced the radioactivity levels of (+)-[^11^C]PMV in all brain regions by 50%. Co-injections with SA4503, haloperidol, (±)-PMV, and (−)-vesamicol also reduced the whole-brain radioactivity levels by 39-57%. Blood radioactivity cleared rapidly. At 5 min after injection, the levels of radioactivity in various organs were 4.66 ± 1.04 (lung), 1.39 ± 0.37 (pancreas), 1.32 ± 0.19 (kidney), 0.93 ± 0.09 (heart), 0.36 ± 0.10 (liver) and 0.11 ± 0.03% ID/g (blood). After 60 min, these levels changed to 2.37 ± 0.42 (lung), 2.00 ± 0.48 (pancreas), 0.81 ± 0.12 (kidney), 0.50 ± 0.05 (heart), 0.65 ± 0.06 (liver) and 0.045 ± 0.005% ID/g (blood). Analysis of (+)-[^11^C]PMV metabolites by HPLC in the plasma and brain samples obtained at 30 min after injection showed that 95% and 21% of (+)-[^11^C]PMV remained in the brain and plasma, respectively.

Ex vivo autoradiography of (+)-[^11^C]PMV (110 MBq/1.4-1.8 nmol (2.97 mCi/1.4-1.8 nmol) in rats showed brain distribution similar to [^11^C]SA4503 at 15 or 30 min after injection (15).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20PMV%20OR%20%28%20%29-p-%5B%2811%29C%5D-methylvesamicol%20OR%20%28methyl%20vesamicol%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20PMV%20OR%20%28%20%29-p-%5B%2811%29C%5D-methylvesamicol%20OR%20%28methyl%20vesamicol%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C%20PMV%20OR%20%28%20%29-p-%5B%2811%29C%5D-methylvesamicol%20OR%20%28methyl%20vesamicol%29%29%20AND%20human)]

No publication is currently available.

## References

1 Kawamura K., Ishiwata K., Tajima H., Ishii S., Matsuno K., Homma Y., Senda M. (2000). In vivo evaluation of [(11)C]SA4503 as a PET ligand for mapping CNS sigma(1) receptors. Nucl Med Biol.
2 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
3 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
4 Skuza G. (2003). Potential antidepressant activity of sigma ligands. Pol J Pharmacol.
5 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
6 Matsuno K., Nakazawa M., Okamoto K., Kawashima Y., Mita S. (1996). Binding properties of SA4503, a novel and selective sigma 1 receptor agonist. Eur J Pharmacol.
7 Kawamura K., Kubota K., Kobayashi T., Elsinga P.H., Ono M., Maeda M., Ishiwata K. (2005). Evaluation of [11C]SA5845 and [11C]SA4503 for imaging of sigma receptors in tumors by animal PET. Ann Nucl Med.
8 van Waarde A., Buursma A.R., Hospers G.A., Kawamura K., Kobayashi T., Ishii K., Oda K., Ishiwata K., Vaalburg W., Elsinga P.H. (2004). Tumor imaging with 2 sigma-receptor ligands, 18F-FE-SA5845 and 11C-SA4503: a feasibility study. J Nucl Med.
9 Langer O., Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
10 Efange S.M. (2000). In vivo imaging of the vesicular acetylcholine transporter and the vesicular monoamine transporter. Faseb J.
11 Efange S.M., Mach R.H., Smith C.R., Khare A.B., Foulon C., Akella S.K., Childers S.R., Parsons S.M. (1995). Vesamicol analogues as sigma ligands. Molecular determinants of selectivity at the vesamicol receptor. Biochem Pharmacol.
12 Shiba K., Yano T., Sato W., Mori H., Tonami N. (2002). Characterization of radioiodinated (-)-ortho-iodovesamicol binding in rat brain preparations. Life Sci.
13 Shiba K., Ogawa K., Mori H. (2005). In vitro characterization of radioiodinated (+)-2-[4-(4-iodophenyl) piperidino]cyclohexanol [(+)-pIV] as a sigma-1 receptor ligand. Bioorg Med Chem.
14 Shiba K., Ogawa K., Ishiwata K., Yajima K., Mori H. (2006). Synthesis and binding affinities of methylvesamicol analogs for the acetylcholine transporter and sigma receptor. Bioorg Med Chem.
15 Ishiwata K., Kawamura K., Yajima K., Qinggeletu, Mori H., Shiba K. (2006). Evaluation of (+)-p-[(11)C]methylvesamicol for mapping sigma(1) receptors: a comparison with [(11)C]SA4503. Nucl Med Biol.